# Trans-4-(N-Methylamino)-4´-{2-[2-(2-[^18^F]fluoro-ethoxy)-ethoxy]-ethoxy}-stilbene

Chemical name: | Trans-4-(N-Methylamino)-4´-{2-[2-(2-[^18^F]fluoro-ethoxy)-ethoxy]-ethoxy}-stilbene
Abbreviated name: | [^18^F]BAY94-9172
Synonym:
Agent category: | Compound
Target: | Aggregates of Amyloid-beta peptide
Target category: | Acceptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions overtime (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of amyloid-beta peptides consisting of 40 to 42 amino acids) and intracellular neurofibrillary tangles (filaments of microtubule-binding hyper-phosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). β-amyloid peptides and tau protein are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various β-amyloid imaging agents have been developed for magnetic resonance imaging (MRI), single photon emission computed tomography (SPECT), and positron emission tomography (PET) (8-13). The binding of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human post-mortem brain tissue and in transgenic mice. Out of these analogues, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) was studied in humans, showing more binding in the brains of patients with AD than in those of healthy people (14). However, [^18^F]FDDNP showed low signal-to-noise ratios for PET imaging, because it is highly lipophilic. N-methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a β-amyloid binding compound based on a series of neutral thioflavin-T derivatives (15), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for the senile plaques in the brain (16). Zhang et al. (17) reported the development of a series of fluorinated polyethylene glycol (PEG) units (n = 2-5) for PET imaging of β-amyloid plaques in the brain. One of them, Trans-4-(N-methylamino)-4´-{2-[2-(2-[^18^F]fluoro-ethoxy)-ethoxy]-ethoxy}-stilbene ([^18^F]BAY94-9172), has been tested in humans.

### Related Resource Links:

- Chapters in MICAD (amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (amyloid (http://www.ncbi.nlm.nih.gov/gene/351))
- Articles in Online Mendelian Inheritance in Man (OMIM) (amyloid (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid))
- Clinical trials (amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid))
- Drug information in FDA (amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20synthesis)]

[^18^F]BAY94-9172 was readily synthesized by standard ^18^F-fluorination of N-BOC-protected mesylate derivative with ([^18^F]KF/Kryptofix 2.2.2), followed by hydrolysis (17). The radiochemical yield was 30% (decay-corrected) at the end of synthesis, and the specific activity was 48.1-55.5 GBq/μmol (1.3 -1.5 Ci/μmol) at the end of synthesis. Radiochemical purity was >99% as determined with high-performance liquid chromatography. Total synthesis time was ~ 90 min. [^18^F]BAY94-9172 exhibited a Log P value of 2.41.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20in%20vitro)]

BAY94-9172 has a binding affinity (K_i_) of 6.7 ± 0.3 nM for aggregated amyloid-beta fibrils (postmortem AD brain homogenates) in competition with [^125^I]IMPY (17). The K_i_ Value for PIB was found to be 2.8 ± 0.5 nM. [^18^F]BAY94-9172 bound to the cortex of postmortem AD brain slices as visualized by autoradiography studies.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20rodentia)]

[^18^F]BAY94-9172 (0.37 MBq, 10 μCi) were injected intravenously into normal mice to study its accumulation into the brain and other organs/tissues at 2, 30, 60 and 120 min after injection (17). [^18^F]BAY94-9172 showed an initial rapid penetration into the brain with 7.8% injected dose (ID)/g at 2 min, with a quick washout (1.6% ID/g at 30 min). The organ with the highest accumulation was the liver, followed by the kidney (13.0% ID/g), lung (3.2% ID/g), heart (2.2% ID/g), and spleen (1.81% ID/g) at 30 min after injection. The radioactivity levels were 2.8% and 1.2% in the blood and bone, respectively. The bone radioactivity increased to 2.7 at 120 min. Ex-vivo autoradiography studies of the brain after injection of [^18^F]BAY94-9172 in the transgenic Tg2576 mice overexpressing β-amyloid plaques were performed. The brain showed a distinctive labeling of β-amyloid plaques and co-staining with thioflavin-S. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20humans)]

Rowe et al. (18) studied 15 patients with mild AD, 15 healthy elderly controls, and five patients with frontotemporal lobar degeneration (FTLD) with [^18^F]BAY94-9172 PET imaging. [^18^F]BAY94-9172 binding was quantified by use of the standardized uptake value ratio (SUVR), which was calculated for the neocortex with the cerebellum as reference region. Widespread neocortical binding was observed in all AD patients., Higher neocortical SUVR was observed in AD patients (2.0 ± 0.3) than in healthy controls (1.3 ± 0.2; P<0.0001) or FTLD patients (1.2 ± 0.2; P=0.009) at 90-120 min after injection with visual interpretation was 100% sensitive and 90% specific for detection of AD.

O’Keefe et al. (19) performed attenuation-corrected whole-body scans at 0, 15, 30, 45, and 60 min after injection of 350 ± 28 MBq of [^11^C]PIB in 6 healthy subjects and at 0, 20, 60, 120, and 180 min after injection of 319 ± 27 MBq of [^18^F]BAY94-9172 in 3 healthy subjects. For [^11^C]PIB, the highest absorbed doses were in the gallbladder wall (44.80 ± 29.30 µGy/MBq), urinary bladder wall (26.30 ± 8.50 µGy/MBq), liver (19.88 ± 3.58 µGy/MBq), and kidneys (12.92 ± 3.37 µGy/MBq). The effective dose (ED) was 5.29 ± 0.66 µSv/MBq. For [^18^F]BAY94-9172, the highest doses were also in the gallbladder wall (132.40 ± 43.40 µGy/MBq), urinary bladder wall (24.77 ± 7.36 µGy/MBq), and liver (39.07 ± 8.31 µGy/MBq). The ED was 14.67 ± 1.39 µSv/MBq. The estimated organ doses for [^11^C]PIB were comparable to those reported in earlier research. With the doses used in published studies (300-700 MBq), the EDs would range from 1.6 to 3.7 mSv. The ED of [^18^F]BAY94-9172 was 30% lower than that of (18)F-FDG and, at the published dose of 300 MBq, would yield an ED of 4.4 mSv.

## NIH Support

AG022559

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
4 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
5 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
6 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
10 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
11 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
12 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
13 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
16 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
17 Zhang W., Oya S., Kung M.P., Hou C., Maier D.L., Kung H.F. (2005). F-18 Polyethyleneglycol stilbenes as PET imaging agents targeting Abeta aggregates in the brain. Nucl Med Biol.
18 Rowe C.C., Ackerman U., Browne W., Mulligan R., Pike K.L., O'Keefe G., Tochon-Danguy H., Chan G., Berlangieri S.U., Jones G., Dickinson-Rowe K.L., Kung H.P., Zhang W., Kung M.P., Skovronsky D., Dyrks T., Holl G., Krause S., Friebe M., Lehman L., Lindemann S., Dinkelborg L.M., Masters C.L., Villemagne V.L. (2008). Imaging of amyloid beta in Alzheimer's disease with 18F-BAY94-9172, a novel PET tracer: proof of mechanism. Lancet Neurol.
19 O'Keefe G.J., Saunder T.H., Ng S., Ackerman U., Tochon-Danguy H.J., Chan J.G., Gong S., Dyrks T., Lindemann S., Holl G., Dinkelborg L., Villemagne V., Rowe C.C. (2009). Radiation Dosimetry of {beta}-Amyloid Tracers 11C-PiB and 18F-BAY94-9172. J Nucl Med.